# ^111^In-Labeled DTPA conjugated anti-c-kit monoclonal antibody 12A8 Fab fragment

Chemical name: | ^111^In-Labeled anti-c-kit monoclonal antibody 12A8 Fab fragment
Abbreviated name: | [^111^In]12A8 Fab
Synonym:
Agent Category: | Antibody fragment
Target: | Proto-oncogene c-Kit; tyrosine-protein kinase kit; mast/stem cell growth factor receptor; CD117
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=c-kit&cmd=DetailsSearch)]

The c-kit (CD 117 antigen or stem cell factor ligand receptor) is a 145-kDa type III glycoprotein receptor tyrosine kinase (TK; encoded by the KIT proto-oncogene) that has a TK at the juxtamembrane position, which is activated when a ligand binds to the extracellular ligand-binding domain of the receptor (1). Almost 70% of gastrointestinal stromal tumors (GISTs) (http://www.cancer.gov/cancertopics/pdq/treatment/gist/HealthProfessional) are known to overexpress a c-kit that has a mutation in exon 11 and produces a constitutively activated TK that promotes the survival and proliferation of cells and leads to the development of a malignant phenotype in the cells of the GISTs (1, 2). The biology and mutations of the c-kit gene and the detection, diagnosis, and chemotherapy of the cancerous GISTs are discussed in detail elsewhere (3, 4). An immunohistochemical method is commonly used to detect the overexpression of c-kit in GIST cancers, but this invasive technique is known to generate variable results (3, 5). In addition, investigators often use positron emission tomography (PET) with ^18^F-fluoro-deoxyglucose to detect, monitor, and assess the response of GISTs to chemotherapy with imatinib, but this radiolabeled probe does not distinguish between GISTs and other cancerous tumors that have an epithelial or lymphatic origin (6).

Recently, the ^111^In-labeled anti–c-kit monoclonal antibody (mAb) 12A8 ([^111^In]12A8) was developed and evaluated for the detection of GISTs with single-photon emission computed tomography (SPECT) in nude mice bearing xenograft tumors that express c-kit (6). However, with [^111^In]12A8 the tumors were first visible on the animals at 48 h postinjection (p.i.) and became clearly visible only at 96 h p.i. This indicated that it was necessary to develop a radiolabeled immunoreagent that would have superior pharmacokinetic properties and yield faster results compared to the ^111^In-labeled mAb. It is well known that mAb fragments such as Fab (~50 kDa) and single-chain antibody fragments (~27 kDa) have superior in vivo pharmacokinetic properties compared to intact mAbs (~150 kDa) (7, 8). In an effort to achieve this goal, a Fab fragment of mAb 12A8 was labeled with ^111^In (to obtain [^111^In]12A8 Fab) and with ^64^Cu (to obtain [^64^Cu]12A8 Fab), and the two probes were evaluated for the detection of tumors that express c-kit in nude mice (2). This chapter describes the SPECT studies performed with [^111^In]12A8 Fab. The detection of tumors that express c-kit with [^64^Cu]12A8 Fab is discussed in a separate chapter of MICAD (www.micad.nih.gov) (9).

### Other Sources of Information

c-kit–Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=c-kit+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human c-kit (also known as Hardy-Zuckerman 4 feline sarcoma viral oncogene-like protein (KIT)) protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/HM015525.1) sequence (Source: NCBI GenBank)

Gene (http://www.ncbi.nlm.nih.gov/nuccore?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=3815) (human c-kit; Gene ID: 3815)

c-kit in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=c-kit)

Signaling events (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200175&source=NATURE&output-format=graphic&ppage=1&genes_a=3815) mediated by c-kit (Source: Pathways Interaction Database)

c-kit–Related clinical trials (http://clinicaltrials.gov/ct2/results?term=c-kit)

Information on c-kit in PubChem Bioassay (http://www.ncbi.nlm.nih.gov/pcassay/?term=c-kit)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20synthesis&cmd=DetailsSearch)]

The source of the 12A8 Fab fragment, its conjugation with N-[(R)-2-amino-3-(p-isothiocyanato-phenyl)propyl]-trans-(S,S)-cyclohexane-1,2-triamine-pentaacetic acid (DTPA), and labeling with ^111^In have been described by Yoshida et al. (2). Using cellulose acetate electrophoresis, the DTPA:Fab ratio of this conjugate was determined to be 2.3. The radiochemical yield and purity of [^111^In]12A8 Fab were reported to be 61.7 ± 15.9% and 98.4 ± 1.3%, respectively, with a specific activity of 1.2 ± 0.3 MBq/μmol (~32.4 ± 8.0 μCi/μmol; n = 3 experiments).

For use as a control, the IgG_1_ 12A8 mAb was also conjugated to DTPA and labeled with ^111^In to obtain [^111^In]IgG as described above (2). Using cellulose acetate electrophoresis, the DTPA:mAb ratio of this conjugate was determined to be 1.1. The radiochemical yield and purity of [^111^In]IgG were reported to be 61.7 ± 15.9% and 98.4 ± 1.3%, respectively, with a specific activity of 3.4 ± 0.9 MBq/μmol (91.8 ± 24.3 μCi/μmol; n = 3 experiments).

For in vitro studies, the 12A8 Fab fragment was labeled with ^125^I using the chloramine-T method (2). The radiochemical yield and purity of [^125^I]12A8 Fab were reported to be 84.4% and 98.0%, respectively, with a specific activity of 37.5 MBq/μmol (~1 mCi/μmol; n = 1 experiment).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20in%20vitro&cmd=DetailsSearch)]

The in vitro cell binding characterization of [^111^In]12A8 IgG, [^111^In]12A8 Fab, and [^125^I]12A8 Fab was performed with human small cell lung cancer cells (SY cells) that express high levels of c-kit (confirmed with Western blot analysis) (2). The cell binding specificities of [^111^In]12A8 IgG, [^111^In]12A8 Fab, and [^125^I]12A8 Fab were determined to be 50.2%, 37.1%, and 39.2%, respectively. The equilibrium dissociation constants of [^111^In]12A8 IgG, [^111^In]12A8 Fab, and [^125^I]12A8 Fab were reported to be 8.0, 18.4, and 18.5 nM, respectively, as determined with a competitive inhibition assay in the presence of increasing concentrations of the unlabeled mAb. The amounts of membrane-bound radioactivity from [^111^In]12A8 Fab and [^125^I]12A8 Fab were observed to decrease with time, but only cells exposed to [^111^In]12A8 Fab showed an increased internalization of the label that reached a maximum of ~15% after incubation for 20 h at 37°C. During the same time, the internalization of [^125^I]12A8 Fab decreased from ~15% at 1 h after incubation to ~8% at 20 h after incubation, and a corresponding increase in the amount of non–protein-bound radioactivity was observed in the growth medium. From this study, the investigators concluded that either free ^125^I or some labeled catabolites of [^125^I]12A8 Fab were released into the cell growth medium during the incubation, which indicated that the radioiodinated mAb fragment was not stable under these study conditions (2).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20rodentia&cmd=DetailsSearch)]

The biodistribution patterns of [^111^In]12A8 IgG and [^111^In]12A8 Fab were studied in nude mice bearing SY cell tumors and A4 cell tumors (NIH-3T3 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1658&Template=cellBiology) that are transfected with the human epidermal growth factor receptor gene and do not express human c-kit) on the left and right thighs, respectively (2). The mice (n = 5 animals/group) were administered the ^111^In-labeled tracers. The animals were euthanized at 24, 48, and 96 h p.i for [^111^In]IgG and at 1, 6, and 12 h p.i. for [^111^In]12A8 Fab to collect the blood, tumor, and other major organs to determine the amount of accumulated radioactivity. Data obtained from this study were standardized to a 20-g body weight mouse and presented as percent of injected dose per gram tissue (% ID/g).

The radioactivity uptake values of [^111^In]12A8 IgG in the A4 tumors was 6.0 ± 0.6% ID/g, 6.5 ± 0.7% ID/g, and 5.6 ± 0.8% ID/g at 24, 48, and 96 h p.i., respectively, compared to values of 15.5 ± 1.9% ID/g, 23.3 ± 2.3% ID/g, and 20.3 ± 1.6% ID/g for the SY tumors at the same time points. The tumor/blood (T/B) ratio for the SY tumors was 1.0 at 24 h p.i. and increased to 2.8 at 96 h p.i. All other organs showed a low uptake of the label that decreased gradually with time. No blocking studies were reported.

With [^111^In]12A8 Fab, the uptake values of the tracer in the A4 tumors were 2.7 ± 0.3% ID/g, 2.1 ± 0.3% ID/g, and 1.3 ± 0.2% ID/g at 1, 6, and 12 h p.i., respectively, compared to 2.7 ± 0.5% ID/g, 4.8 ± 0.8% ID/g, and 4.4 ± 1.2% ID/g (P <0.01 for the latter two values) at the same time points for the SY tumors. The T/B ratios for the SY tumors were 0.3, 3.3, and 9.7 at 1, 6, and 12 h, respectively. All other organs except the kidneys showed a decrease in radioactivity with time. The accumulation of tracer was observed to be 52.5 ± 5.0% ID/g in the kidneys at 6 h p.i. and decreased to 35.8 ± 4.2% ID/g at 12 h p.i., which indicated that the radioactivity was excreted primarily through the renal route. No blocking studies were reported.

From these studies, the investigators concluded that [^111^In]12A8 Fab was suitable to detect GISTs in rodents (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Aubin F., Blanke C.D. (2011). Metastatic gastrointestinal stromal tumors. Cancer Chemother Pharmacol.
2 Yoshida C., et al. (2011). Development of positron emission tomography probe of 64Cu-labeled anti-C-kit 12A8 Fab to measure protooncogene C-kit expression. Nucl Med Biol.
3 Corless C.L., Heinrich M.C. (2008). Molecular pathobiology of gastrointestinal stromal sarcomas. Annu Rev Pathol.
4 Wang W.L., et al. (2011). Mechanisms of resistance to imatinib and sunitinib in gastrointestinal stromal tumor. Cancer Chemother Pharmacol.
5 Miettinen M., Lasota J. (2005). KIT (CD117): a review on expression in normal and neoplastic tissues, and mutations and their clinicopathologic correlation. Appl Immunohistochem Mol Morphol.
6 Sogawa C., et al. (2010). C-kit-targeted imaging of gastrointestinal stromal tumor using radiolabeled anti-c-kit monoclonal antibody in a mouse tumor model. Nucl Med Biol.
7 Accardi L., Di Bonito P. (2010). Antibodies in single-chain format against tumour-associated antigens: present and future applications. Curr Med Chem.
8 Marik J., Junutula J.R. (2011). Emerging role of immunoPET in receptor targeted cancer therapy. Curr Drug Deliv.
9 Chopra, A., 64Cu-Labeled anti-c-kit monoclonal antibody 12A8 Fab fragment. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.